# Cy5.5-Conjugated anti-human CD31 monoclonal antibody

Chemical name: | Cy5.5-Conjugated anti-human CD31 monoclonal antibody | [image]
Abbreviated name: | Cy5.5-anti-hCD31 MAb | [image]
Synonym: | | [image]
Agent Category: | Antibody | [image]
Target: | CD31 | [image]
Target Category: | Binding | [image]
Method of detection: | Fluorescence imaging | [image]
Source of signal / contrast: | Cy5.5 | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of Cy5.5-anti-hCD31 MAb.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CD31)]

The CD31 molecule, also known as the platelet endothelial cell (EC) adhesion molecule 1, is a 130-kD transmembrane glycoprotein that is a member of the immunoglobulin superfamily. This glycoprotein is expressed primarily on the EC intercellular junctions in the vascular system, but it is also expressed to a varying extent on other cell types (1, 2). The ECs are believed to play a major role in a variety of physiological processes such as coagulation, vascular tone, inflammation, and angiogenesis (1). Although CD31 is expressed in several leukocyte cell subtypes and in platelets, it is considered to be a reliable marker for tumor vasculature (3, 4). Runnels et al. showed that fluorescence-labeled rat anti-mouse CD31 monoclonal antibodies (MAbs) targeting the CD31 molecule could be used for the in vivo imaging of EC dynamics in mice (5). The investigators showed that the MAbs could stain the ECs in the vascular wall for a period of 24 to 48 h after administration. On the basis of these observations, Bogdanov et al. designed a similar study using the anti-human CD31 MAb labeled with the near-infrared fluorescent dye Cy5.5 (Cy5.5 anti-hCD31) to investigate the detection of human EC-lined blood vessels developed in an animal model using human umbilical vein EC (HUVEC) Matrigel implants (6). To perform this study the investigators assumed that the human anti-CD31 MAb did not cross-react with the mouse ECs and had a high affinity for the targeted marker protein, that the CD31 was constitutively expressed on the surface of ECs, and that the MAb was internalized at a slow rate.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti+CD31+monoclonal+antibody+Cy5%2E5+synthesis)]

The anti-human CD31 MAb used in the studies was received as a gift from a commercial source (6). The MAb, in 0.1 M sodium bicarbonate buffer (pH 8.7), was mixed with the N-hydroxysuccinimide monocarboxylic (NHS) ester of Cy5.5 (Cy5.5-NHS) in dimethylsulfoxide (in a dye:MAb molar ratio of 10:1). The mixture was incubated for 30 min (temperature not reported), and the labeled protein was purified with spin-chromatography on a mini spin column. A similar procedure was used to respectively conjugate a mouse anti-human E-selectin MAb fragment F(ab’)_2_ and a rat anti-mouse CD31 MAb with Alexa Fluor 488-NHS ester. Purification of these labeled MAbs was performed as described above. Ulex europaeus or Lycopersicon esculentum lectins were also respectively conjugated with Cy5.5-NHS and processed as given above. The purity and storage conditions used for the various conjugated MAbs and lectins were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti+CD31+monoclonal+antibody+Cy5%2E5+in+vitro)]

To test the fluorescent labeling of the two lectins, which have specificity for acetylglucosamine (L. esculentum) and α-L-fucose (U. europaeus), HUVEC and mouse vascular ECs (MVEC) were grown on glass-coverslip chambers and double-stained with the Cy5.5-labeled lectins and the anti-human or anti-mouse CD31 MABs (6). Both lectins stained the respective cells (HUVEC with the U. europaeus lectin and the MVEC with the L. esculentum lectin) as expected; however, the lectins did not show any specificity because the labeled lectins showed a cross-reactivity for both cell types. The species-specific anti-CD31 antibodies showed a homogeneous staining of the cells, indicating that the primary ECs were pure and did not contain any contaminating cells that would result in cross-staining with the labeled lectins. No competing studies with the unlabeled lectins or with the MAbs were reported.

In another study, the HUVEC cells were double-stained with the Cy5.5-anti-human CD31 MAb and the Alexa Fluor 488–conjugated anti-E-selectin MAb fragment F(ab’)_2_. Near-infrared fluorescent confocal microscope imaging revealed that the anti-human CD31 MAb (red fluorescence) was associated primarily with the intracellular junctions of the cells and that the E-selectin MAb (green fluorescence) showed little binding to the cells. Treatment of the cells with interleukin-1β (a pro-inflammatory cytokine; E-selectin has a role in inflammation) resulted in rapid cellular internalization of the E-selectin–labeled MAb, but there was only a little internalization of the anti-human CD31-labeled MAb under these conditions. Pre-exposure of the cells to N-ethylmaleimide or incubation (total incubation time not reported) at 4°C was reported to completely block internalization of either labeled MAb.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CD31+MAb+Cy5%2E5+Rodentia)]

Matrigel supplemented with growth factors (fibroblast growth factor and vascular endothelial growth factor) and mixed with or without HUVEC (to serve as controls) was injected into the right and left posterior flanks, respectively, of nu/nu mice to establish human cell-lined blood vessels in the animals (6). After approximately 3 to 4 weeks, the animals (n = 3 animals/group) were intravenously injected with the Cy5.5-anti-human CD31 MAb. Near-infrared imaging of the animals immediately after administration of the labeled MAb showed that the mouse body fluorescence was increased during the initial 5 min, followed by a gradual decrease as the imaging probe cleared from circulation. Approximately 2.5 h after injection, animals injected with the HUVEC Matrigel showed an increased fluorescence with a signal/noise ratio of 1.6–1.8 compared to the control animals. A histological examination with near-infrared fluorescence microscopy of frozen sections obtained from animals injected with Matrigel with or without HUVECs showed that the endothelium-lined blood vessels were visible only in animals with HUVEC Matrigel. No such structures were visible in frozen sections from the control animals.

The investigators triple-stained the HUVEC Matrigel implants with the Cy5.5-anti-human CD31 MAb, the Alexa Fluor 488–anti-mouse CD31 MAb, and 4,6'-diamidino-2-phenylindole (DAPI; blue fluorescent stain for nuclei) (6). A network of blood vessels almost entirely positive for the anti-human CD31 MAb and DAPI was observed in the HUVEC Matrigel sections. No staining with the labeled anti-mouse CD31 MAb was observed in these sections.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CD31+MAb+Cy5%2E5+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CD31+MAb+Cy5%2E5+Non+Primate+Mammals)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CD31+MAb+Cy5%2E5+Human+Studies)]

No references are currently available.

## Supplemental Information

### NIH Support

Some studies presented in this chapter were funded by National Institutes of Health grants RO1 EB000858 and EB000664.

### References

1 Pusztaszeri M.P., Seelentag W., Bosman F.T. (2006). Immunohistochemical expression of endothelial markers CD31, CD34, von Willebrand factor, and Fli-1 in normal human tissues. J Histochem Cytochem.
2 Woodfin A., Voisin M.B., Nourshargh S. (2007). PECAM-1: a multi-functional molecule in inflammation and vascular biology. Arterioscler Thromb Vasc Biol.
3 (1998). De Young, B.R., H.F. Frierson, Jr., M.N. Ly, D. Smith, and P.E. Swanson, CD31 immunoreactivity in carcinomas and mesotheliomas. Am J Clin Pathol.
4 Fox S.B., Gatter K.C., Bicknell R., Going J.J., Stanton P., Cooke T.G., Harris A.L. (1993). Relationship of endothelial cell proliferation to tumor vascularity in human breast cancer. Cancer Res.
5 Runnels J.M., Zamiri P., Spencer J.A., Veilleux I., Wei X., Bogdanov A., Lin C.P. (2006). Imaging molecular expression on vascular endothelial cells by in vivo immunofluorescence microscopy. Mol Imaging.
6 Bogdanov A.A., Lin C.P., Kang H.W. (2007). Optical imaging of the adoptive transfer of human endothelial cells in mice using anti-human CD31 monoclonal antibody. Pharm Res.